# ^64^Cu-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-conjugated IRDye 800CW (a near-infrared fluorescence dye) coupled to mAb7, an anti-epithelial cell adhesion molecule monoclonal antibody

Chemical name: | ^64^Cu-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-conjugated IRDye 800CW (a near-infrared fluorescence dye) coupled to mAb7, an anti-epithelial cell adhesion molecule monoclonal antibody
Abbreviated name: | [^64^Cu]DOTA-IRDye 800CW-mAb7
Synonym:
Agent Category: | Compound
Target: | Epithelial cell adhesion molecule (EpCAM)
Target Category: | Antigen
Method of detection: | Near-infrared fluorescence (NIRF) imaging; positron emission tomography (PET)
Source of signal / contrast: | Multimodal: IRDye 800CW (near-infrared fluorescence (NIRF) imaging); ^64^Cu (PET)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=radiolabeled%20antibodies&cmd=DetailsSearch)]

Antibodies and their derivatives directed against a variety of molecular targets such as receptors and antigens have been conjugated to positron-emitting radionuclides (e.g., ^64^Cu, ^89^Zr, ^68^Ga, etc.) and used with positron emission tomography (PET) for the successful visualization of cancerous tumors (1). However, although PET is a high-specificity imaging modality that can be used to detect and quantify a target, the major limitations of using this technique is that it is expensive, produces low spatial resolution, and cannot be used for the accurate staging of cancer (2) or for real-time imaging during surgical resection of a cancerous tumor (3). In this regard, near-infrared fluorescence (NIRF) imaging is relatively inexpensive, has a high sensitivity and spatial resolution, does not require the use of radionuclides, and can be used to view surgical resection of neoplastic tumor in real time (3). Therefore, a combination of PET and NIRF capabilities within the same imaging agent should greatly improve the preclinical or clinical investigative potential of a probe because each modality will balance the deficiency of the other (4). On the basis of this hypothesis, Zhang et al. labeled an anti-CD105 monoclonal antibody (mAb; TR105) with ^64^Cu, coupled the complex to IRDye 800CW, a NIRF dye, and then successfully used the dual-labeled mAb with PET and NIRF techniques to detect tumors that overexpressed CD105 in rodents (5).

Ghosh et al. coupled a bifunctional metal-chelating agent (1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)) to a NIRF dye (IRDye 800CW; DOTA-IRDye 800CW) and labeled the complex with either ^68^Ga or ^64^Cu ([^68^Ga/^64^Cu]DOTA-IRDye 800CW) (6). The investigators studied the biodistribution of [^68^Ga/^64^Cu]DOTA-IRDye 800CW in normal nude mice with PET and NIRF imaging, and they determined that [^64^Cu]DOTA-IRDye 800CW had superior tissue distribution profile and fluorescence characteristics compared with the ^68^Ga-labeled dye. For another study, DOTA-IRDye 800CW was coupled to mAb7, an anti-epithelial cell adhesion molecule (EpCAM) monoclonal antibody, and labeled with ^64^Cu ([^64^Cu]DOTA-IRDye 800CW-mAb7) (6). The biodistribution of [^64^Cu]DOTA-IRDye 800CW-mAb7 was investigated in nude mice bearing tumors derived from PC3 cells (http://www.atcc.org/Products/All/CRL-1435.aspx) transfected with the DsRed fluorescent protein gene reporter (PC3-DsRed cells; PC3 cells are known to express the EpCAM antigen) (6).

### Related Resource Links

Multimodal agents (http://www.ncbi.nlm.nih.gov/books?term=Multimodal%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D%20AND%20table%5Btype%5D&cmd=DetailsSearch) in MICAD

EpCAM (http://clinicaltrials.gov/ct2/results?term=Epithelial+cell+adhesion+molecule&Search=Search)-related clinical trials

Human EpCAM (http://www.ncbi.nlm.nih.gov/gene/4072) in Gene Database; Gene ID: 4072

EpCAM in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/185535))

Protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/218505669) of human EpCAM

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA%20IRDye%20CW800%20synthesis&cmd=DetailsSearch)]

The synthesis of DOTA-IRDye 800CW (for structure see (6)), [^68^Ga/^64^Cu]DOTA-IRDye 800CW, and [^64^Cu]DOTA-IRDye 800CW-mAb7 has been described by Ghosh et al. (6). The identity of the various conjugates was confirmed with mass spectroscopy, and the purity of DOTA-IRDye CW800 was >95% as determined with high-performance liquid chromatography (HPLC). Each compound was freeze-dried and stored at −20°C until required.

Each molecule of mAb7 was reported to be coupled to 2.8 molecules of the chelator/NIRF dye complex as determined with ^64^Cu labeling and fluorescence spectrophotometric methods (6).

The radiochemical yield (RCY) of [^64^Cu]DOTA-IRDye 800CW-mAb7 was 51.9%; the radiochemical purity (RCP) of the dual-labeled mAb7 was not reported (6). The specific activity (SA) of [^64^Cu]DOTA-IRDye 800CW-mAb7 was reported to be ~37 MBq/0.66 nmol (1.0 mCi/0.66 nmol). The RCY, RCP, and SA of [^68^Ga/^64^Cu]DOTA-IRDye 800CW were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA%20IRDye%20CW800%20in%20vitro%20studies&cmd=DetailsSearch)]

Conjugation of DOTA to IRDye 800CW was reported to decrease the extinction coefficient (EC) and the quantum yield (QY) of the parent dye by 8% and 3%, respectively (6). In addition, labeling of DOTA-IRDye 800CW with ^64^Cu reduced the EC and the QY of the compound by ~20%, whereas labeling of the conjugate with ^68^Ga decreased these parameters by 35% and 24.2%, respectively. Compared with the native IRDye 800CW, the relative fluorescence brightness (RB) of DOTA-IRDye 800CW was lower by 11.1%; labeling of the DOTA conjugate with ^64^Cu or ^68^Ga further reduced the RB by 33.3% and 50.5%, respectively (6). This suggested that the ^64^Cu-labeled conjugate was superior to the ^68^Ga-labeled tracer for use with NIRF imaging.

The in vitro stability of [^68^Ga]DOTA-IRDye 800CW and [^64^Cu]DOTA-IRDye 800CW was determined by incubating the dual-labeled conjugates in 50% mouse serum for up to 24 h at 37°C (6). After incubation for 3 h, 97 ± 1.0% of [^68^Ga]DOTA-IRDye 800CW was intact as determined with radio-HPLC. Incubation of [^64^Cu]DOTA-IRDye 800CW under the same conditions for 24 h revealed that 93.7 ± 4.2% of the labeled conjugate was unchanged (the stability of the ^68^Ga-labeled conjugate at the 24-h timepoint was not reported).

Because [^64^Cu]DOTA-IRDye 800CW had a superior fluorescence and stability compared with [^68^Ga]DOTA-IRDye 800CW, only the former radiolabeled conjugate was used for all subsequent studies (6).

The uptake of [^64^Cu]DOTA-IRDye 800CW-mAb7 was studied in PC3-DsRed cells as described by Ghosh et al. (6). The cells accumulated ~21% of the total added radioactivity after 24 h compared with an accumulation of ~2.0% and ~6.0% of the total added label for [^64^Cu]DOTA-IRDye 800CW and an isotype control ^64^Cu-labeled mAb (this mAb was not identified), respectively. This indicated that the dual-labeled mAb7 conjugate had a higher binding specificity (and internalization) for the cells compared with [^64^Cu]DOTA-IRDye 800CW.

A flow cytometry analysis of [^64^Cu]DOTA-IRDye 800CW-mAb7 with PC3-DsRed cells showed that a median 80.8% of the cells bound the dual-labeled mAb (6). This indicated that chemical modification of the mAb did not alter its binding specificity to the EpCAM antigen expressed on the PC3-DsRed cells (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA%20IRDye%20CW800%20rodentia&cmd=DetailsSearch)]

The tissue distribution of non-targeted [^68^Ga]DOTA-IRDye 800CW and [^64^Cu]DOTA-IRDye 800CW was studied in normal C57BL/6 mice (n = 3 animals/tracer) (6). The rodents (under anesthesia) were intravenously injected with 5.55–7.4 MBq (150–200 μCi) of either radiolabeled compound, and dynamic PET images of the animals were acquired for the next 30 min. Region-of-interest analysis was performed on the images to obtain the percent of injected dose per gram (% ID/g) values for the different organs of interest (6). In addition, time-activity curves (TACs) were generated from the PET images for select organs. Control animals (n = 3 mice/agent) were injected with either [^68^Ga]-IRDye 800CW or [^64^Cu]-IRDye 800CW. After PET imaging, whole-body NIRF images of the animals were acquired at 1 h postinjection (p.i.), 4 h p.i., and 24 h p.i. The TACs showed that with [^64^Cu]-IRDye 800CW the amount of radioactivity in the heart peaked at 2 min p.i., and it was approximately three-fold higher than with [^68^Ga]-IRDye 800CW. With both tracers, the label was gradually lost from all the other tissues, except for the liver. There was a gradual accumulation of radioactivity in the kidneys with [^64^Cu]-IRDye 800CW, and at 30 min p.i. the accumulation reached ~10.0% ID/g (maximum); with [^68^Ga]-IRDye 800CW, however, the label was gradually lost from this organ by 30 min p.i.

NIRF images of animals injected with [^68^Ga]DOTA-IRDye 800CW or [^64^Cu]DOTA-IRDye 800CW were compared with those obtained from animals injected with the unlabeled IRDye 800CW dye (6). Imaging at 1 h p.i. showed that the fluorescence signal generated from the bladder of animals injected with [^68^Ga]DOTA-IRDye 800CW was higher than that obtained from mice injected with either unlabeled IRDye 800CW alone or [^64^Cu]DOTA-IRDye 800CW; with the latter radiochemical, the accumulation of dye in the bladder was more gradual. With [^68^Ga]DOTA-IRDye 800CW, no fluorescence was detected in the different organs by 24 h p.i.; with [^64^Cu]DOTA-IRDye 800CW, a high signal was detected in the kidneys, bladder, and liver. This data indicated that the radioactivity and dye from [^68^Ga]DOTA-IRDye 800CW were rapidly cleared from the system of the normal mice primarily through the renal route. However, the clearance of [^64^Cu]DOTA-IRDye 800CW was through both the renal and the hepatobiliary routes.

The biodistribution of [^64^Cu]DOTA-IRDye 800CW was studied in normal athymic nude mice (n = 3 animals/time point) (6). The animals were injected with 740 kBq (20 μCi) of the radiolabeled compound through the tail vein, and the rodents were euthanized at 1 h p.i. and 24 h p.i. to determine the amount of radioactivity accumulated in the organs of interest (in the study described above, the biodistribution of [^64^Cu]DOTA-IRDye 800CW was studied up to only 30 min p.i. with PET imaging). At 1 h p.i., the label was detected mainly in the liver (7.53 ± 0.58% ID/g) and the kidneys (4.6 ± 0.63% ID/g), and all other organs showed <2.0% ID/g accumulation of the tracer. By 24 h p.i., the amount of radioactivity in the kidneys and the liver decreased by 51.3% and 26.8%, respectively. These results indicated that [^64^Cu]DOTA-IRDye 800CW showed very little nonspecific binding in normal tissues (6).

The biodistribution and tumor-targeting properties of [^64^Cu]DOTA-IRDye 800CW-mAb7 were investigated in athymic nude mice bearing PC3-DsRed cell lesions (number of animals not reported) (6). The animals were injected with 7.4 MBq (75 μCi) of either [^64^Cu]DOTA-IRDye 800CW or [^64^Cu]DOTA-IRDye 800CW-mAb7; PET/computed tomography (CT), DsRed (to confirm presence of tumors), and NIRF images of the mice were acquired at 1 h p.i., 20 h p.i., and 40 h p.i. The animals were euthanized after the last imaging session to remove the organs of interest and to confirm any correlation between the DsRed and NIRF signals. In addition, accumulated radioactivity was counted in each organ to quantify (% ID/g) the amount of label present in the various tissues. At 40 h p.i., the tumors were easily visible in the animals only with DsRed and NIRF imaging; whole-body microPET/CT imaging did not show the lesions very clearly (this was attributed to the small size of the lesions). With [^64^Cu]DOTA-IRDye 800CW-mAb7, the NIRF signal observed in the excised tumor correlated with the DsRed signal obtained from the lesion; with [^64^Cu]DOTA-IRDye 800CW, no NIRF signal was generated in the tumor. The NIRF and DsRed signals were also observed in the liver and kidneys, but these agents generated almost no signal in the other tissues. Quantification of radioactivity from [^64^Cu]DOTA-IRDye 800CW-mAb7 in the various tissues showed that the amount of label in the tumor, liver, and kidneys was 4.48 ± 0.75% ID/g, 9.03 ± 0.36% ID/g, and 3.25 ± 0.22% ID/g, respectively. With [^64^Cu]DOTA-IRDye 800CW, the uptake of tracer in the tumor, liver, and kidneys was 1.26 ± 0.84% ID/g, 4.39 ± 0.75% ID/g, and 2.07 ± 0.29% ID/g, respectively. This showed that the conjugation of [^64^Cu]DOTA-IRDye 800CW to mAb7 enabled higher accumulation of the label in the lesion.

From these studies, the investigators concluded that further optimization and validation of the radionuclide/chelator/fluorescence dye scaffold is necessary before such dual-modality mAb-targeted imaging agents can be used in the clinic (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA%20IRDye%20CW800%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA%20IRDye%20CW800%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA%20IRDye%20CW800%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported in part by National Institutes of Health Grant U54 CA136404.

## References

1 van Dongen G.A., Poot A.J., Vugts D.J. (2012). PET imaging with radiolabeled antibodies and tyrosine kinase inhibitors: immuno-PET and TKI-PET. Tumour Biol.
2 Seevaratnam R., Cardoso R., McGregor C., Lourenco L., Mahar A., Sutradhar R., Law C., Paszat L., Coburn N. (2012). How useful is preoperative imaging for tumor, node, metastasis (TNM) staging of gastric cancer? A meta-analysis. Gastric Cancer.
3 Pysz M.A., Gambhir S.S., Willmann J.K. (2010). Molecular imaging: current status and emerging strategies. Clin Radiol.
4 Thorp-Greenwood F.L., Coogan M.P. (2011). Multimodal radio- (PET/SPECT) and fluorescence imaging agents based on metallo-radioisotopes: current applications and prospects for development of new agents. Dalton Trans.
5 Zhang Y., Hong H., Engle J.W., Yang Y., Theuer C.P., Barnhart T.E., Cai W. (2012). Positron emission tomography and optical imaging of tumor CD105 expression with a dual-labeled monoclonal antibody. Mol Pharm.
6 Ghosh S.C., Ghosh P., Wilganowski N., Robinson H., Hall M.A., Dickinson G., Pinkston K.L., Harvey B.R., Sevick-Muraca E.M., Azhdarinia A. (2013). Multimodal chelation platform for near-infrared fluorescence/nuclear imaging. J Med Chem.